# Microbubbles coated with biotinylated rabbit anti-mouse vascular endothelial growth factor receptor 2 (VEGFR-2) monoclonal antibody

Chemical name: | Microbubbles coated with rabbit anti-mouse vascular endothelial growth factor receptor 2 (VEGFR-2) monoclonal antibody
Abbreviated name: | MB_vegfr2_
Synonym:
Agent Category: | Antibody
Target: | Vascular endothelial growth factor receptor 2 (VEGFR-2)
Target Category: | Receptor
Method of detection: | Ultrasound
Source of signal / contrast: | Microbubbles
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Ultrasound%20microbubbles&cmd=DetailsSearch)]

Angiogenesis, the development of new vasculature from pre-existing blood vessels (for details see Carmeliet and Jain (1)), is essential for the development, maintenance, progression, and metastasis of neoplastic tumors (2). Therefore, angiogenesis is considered to be the hallmark of cancerous tumors, and early detection of this process can facilitate the initiation of treatment and management of the disease (3). Although there are several known pro-angiogenic biomarkers, among these only vascular endothelial growth factor receptor 2 (VEGFR-2) (4), α_V_β_3_ integrin (5), and endoglin (6) are well characterized and are overexpressed in many cancerous tumors, such as those of the breast, ovaries, and the pancreas (3). The VEGFR-2 mediates its effects through a family of receptor tyrosine kinases that promote the mitogenesis, survival, differentiation, migration, and vascular permeability of endothelial cells (7). The α_V_β_3_ integrins are heterodimeric cell adhesion molecules that can bind several different endogenous ligands such as fibronectin, von Willebrand factor, fibrinogen, etc., and assist with the survival and migration of cancerous cells, which increases the invasive potential of these cells, and promotes angiogenesis in tumors (8). Endoglin (CD105) is a co-receptor of the transforming growth factor beta (TGF-β) and co-modulates the different activities, including angiogenesis, of the activated TGF-β receptor (9).

Little information is available regarding the expression of the different angiogenic markers during the progression of a tumor from a small size to a larger size. Noninvasive visualization of angiogenic markers that are overexpressed during initial stages of the neoplasia can facilitate early detection and treatment of the disease (3). For this, Deshpande et al. developed a series of microbubble (MB; perfluorocarbon gas enclosed within spherical lipid shells harboring streptavidin moieties to bind biotinylated monoclonal antibodies (mAb) directed toward specific targets) based contrast agents that were coated with specific antibodies targeted to α_V_β_3_ integrin VEGFR 2 (MB_vegfr2_), (MB_integrin_), and endoglin (MB_endoglin_), respectively (3). The targeted MBs were then used with ultrasound imaging to determine the expression of the angiogenic biomarkers during the growth of human ovarian (SKOV3 cells (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-77&Template=cellBiology)), human breast (MDA-MB-361 cells (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-27&Template=cellBiology)), and human pancreatic (MiaPaCa2 cells (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-1420&Template=cellBiology)) cell line xenograft tumors in mice. This chapter describes the studies performed with MB_vegfr2_. Studies performed with MB_endoglin_ and MB_integrin_ are described in separate chapters of MICAD (www.micad.nih.gov) (10, 11).

### Related Resource Links

VEGFR 2 related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=VEGFR+2+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Human VEGFR, variant 1, protein and mRNA sequences (http://www.ncbi.nlm.nih.gov/nuccore/NM_002019.4)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=VEGFR) related to VEGFR

VEGF and VEGFR signaling network (http://pid.nci.nih.gov/search/pathway_landing.shtml?what=graphic&jpg=on&pathway_id=200107&source=NATURE&output-format=graphic&ppage=1&genes_a=3791) (from Pathways Interaction Database)

United States Food and Drug Administration approved anti-VEGF drugs (http://dailymed.nlm.nih.gov/dailymed/search.cfm?startswith=Vascular+endothelial+growth+factor+receptor)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20synthesis)]

The synthesis of MB_vegfr2_ has been described in detail by Deshpande et al. (3). Briefly, the MBs were obtained as a freeze-dried preparation from a commercial source and reconstituted in 1 mL sterile 0.9% sodium chloride. Subsequently, 5 × 10^7^ of the reconstituted MBs were incubated with 5 μg biotinylated anti-mouse VEGFR 2 mAb for 10 min at room temperature to obtain MB_vegfr2_. A similar procedure was used to obtain MB_endoglin_ and MB_integrin_. For use as controls, another batch of MBs was linked to biotinylated rabbit immunoglobulin G antibodies (MB_control_). The procedure used to remove excess mAb, if any, from the final preparations was not reported. The average number of antibody molecules bound per square micrometer of the MBs of each preparation was reported to be ~7,600 as determined with fluorescence-activated cell sorter analysis (3).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MB%20endoglin%20in%20vitro%20studies&cmd=DetailsSearchhttp://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20in%20vitro)]

A parallel plate flow chamber cell-binding assay with SVR cells (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-2280&Template=cellBiology) (the high expression of VEGFR 2 and the other angiogenic biomarkers by these cells was confirmed with immunofluorescence staining) revealed that, compared to MB_control_, a significantly higher (P = 0.003) amount of MB_vegfr2_ bound to these cells (3). Little or no binding of these MBs was observed with control cells (4T1 cells (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-2539&Template=cellBiology)) that did not express any of the angiogenic biomarkers. An overall significantly positive correlation (ρ = 0.83; P = 0.042) was observed between the number of MBs that attached to the SVR cells and the expression of VEGFR 2 by the cells. Pre-incubation of the SVR cells with the rabbit anti-mouse VEGFR 2 mAb was reported to block the binding of MB_vegfr2_.

An ex vivo immunofluorescence study of the tumor sections showed that VEGFR 2 in the cells was colocalized with CD31, a biomarker specific for endothelial cells (3). This indicated that the in vivo ultrasound signal obtained from the cancerous lesions was indeed generated by the MB_vegfr2_ bound to the VEGFR 2 receptors expressed by the cells in the tumors. In addition, a good correlation (ρ = 0.63) was evident between the in vivo ultrasound imaging signal and the ex vivo expression level of VEGFR 2 in the tumors (P = 0.05) (3).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MB%20endoglin%20rodentia&cmd=DetailsSearch)]

The expression of VEGFR 2 was investigated using MB_vegfr2_ with ultrasound imaging during the different growth size based stages (small, 50–150 mm^3^; medium, 150–250 mm^3^; large, >250 mm^3^) of subcutaneous breast, ovarian, and pancreatic cell line xenograft tumors in mice (n = 3 animals/tumor type) as described by Deshpande at al (3). In addition, the expression of VEGFR-2 was compared with that of endoglin and α_V_β_3_ integrin in these lesions.

Using the different MB based mAbs, ultrasound visualization of small and medium-sized breast cell line xenograft tumors in mice showed that the lesions expressed approximately the same levels (P = 0.70) of VEGFR-2 and α_V_β_3_ integrin, but the expression of endoglin in the neoplasms was significantly higher (P ≤ 0.04) than that of either VEGFR-2 or α_V_β_3_ integrin (3). All the three angiogenic markers had a similar level of expression in the large tumors of the breast cell line (P ≥ 0.08).

Ultrasound imaging with the different MB-antibody preparations showed that the expression of both VEGFR-2 and α_V_β_3_ integrin was lower than that of endoglin (P ≤ 0.04) in all sizes of the ovarian cell line xenograft tumors (3). No significant difference (P ≥ 0.40) was observed in the expression level of VEGFR-2 and α_V_β_3_ integrin in the different sizes of the ovarian cell line lesions.

The small pancreatic cell line xenograft tumors were shown to express lower levels of either VEGFR-2 (P = 0.07) or endoglin (P = 0.15) compared with α_V_β_3_ integrin (3). No significant difference in the expression level of the three angiogenic markers was observed in the medium-sized tumors. Compared with VEGFR 2 (P = 0.22) the large pancreatic cell line lesions showed a significantly higher expression of endoglin (P = 0.01).

From these studies, the investigators concluded that the expression level of the different angiogenic markers varies with the growth stage of the tumor (3). They also concluded that targeted MB-based contrast agents can be used with ultrasound imaging to detect tumors in the early stages of growth in mice.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MB%20endoglin%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MB%20endoglin%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MB%20endoglin%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No Supplemental Information is currently available.

## References

1 Carmeliet P., Jain R.K. (2011). Molecular mechanisms and clinical applications of angiogenesis. Nature.
2 De Bock K., Mazzone M., Carmeliet P. (2011). Antiangiogenic therapy, hypoxia, and metastasis: risky liaisons, or not?. Nat Rev Clin Oncol.
3 Deshpande N., Ren Y., Foygel K., Rosenberg J., Willmann J.K. (2011). Tumor angiogenic marker expression levels during tumor growth: longitudinal assessment with molecularly targeted microbubbles and US imaging. Radiology.
4 Shibuya M., Claesson-Welsh L. (2006). Signal transduction by VEGF receptors in regulation of angiogenesis and lymphangiogenesis. Exp Cell Res.
5 Cai W., Chen X. (2006). Anti-angiogenic cancer therapy based on integrin alphavbeta3 antagonism. Anticancer Agents Med Chem.
6 Nassiri F., Cusimano M.D., Scheithauer B.W., Rotondo F., Fazio A., Yousef G.M., Syro L.V., Kovacs K., Lloyd R.V. (2011). Endoglin (CD105): a review of its role in angiogenesis and tumor diagnosis, progression and therapy. Anticancer Res.
7 Koch S., Tugues S., Li X., Gualandi L., Claesson-Welsh L. (2011). Signal transduction by vascular endothelial growth factor receptors. Biochem J.
8 Wu G., Wang X., Deng G., Wu L., Ju S., Teng G., Yao Y., Liu N. (2011). Novel peptide targeting integrin alphavbeta3-rich tumor cells by magnetic resonance imaging. J Magn Reson Imaging.
9 Perez-Gomez E., Del Castillo G., Juan Francisco S., Lopez-Novoa J.M., Bernabeu C., Quintanilla M. (2010). The role of the TGF-beta coreceptor endoglin in cancer. ScientificWorldJournal.
10 Chopra, A., Microbubbles coated with biotinylated rabbit anti-mouse endoglin monoclonal antibody. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
11 Chopra, A., Microbubbles coated with biotinylated rabbit anti-mouse alphaV beta3 integrin monoclonal antibody. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.